# N-Benzyl-N-ethyl-2-[7,8-dihydro-7-(2-[^18^F]fluoroethyl)-8-oxo-2-phenyl-9H-purin-9-yl]acetamide

Chemical name: | N-Benzyl-N-ethyl-2-[7,8-dihydro-7-(2-[^18^F]fluoroethyl)-8-oxo-2-phenyl-9H-purin-9-yl]acetamide
Abbreviated name: | [^18^F]FEAC
Synonym:
Agent category: | Compound
Target: | Peripheral-type benzodiazepine receptor (PBR), also known as translocator protein (TSPO)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%5BAll%20Fields%5D)]

Benzodiazepines are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been designated as central benzodiazepine receptors (CBR) and peripheral benzodiazepine receptors (PBR). PBR is also known as translocator protein (TSPO). The CBR is found exclusively in the central nervous system on the membranes of neurons and is coupled to the γ-aminobutyric acid receptor/chloride channel (3). In contrast, the PBR is a mitochondrial protein found in brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4). The brain has lower levels of PBR than do the peripheral tissues. Both glial cells and macrophages contain high levels of PBR (5-7). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage that accompanies several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBRs have been studied in vivo with positron emission tomography (PET) using 1-(2-chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide ([^11^C]PK11195), an isoquinoline carboxamide with specific PBR antagonistic activity (8). [^11^C]PK11195 has been developed as a PET agent for non-invasive studies of microglia and macrophage activation in the brain, lung, and heart. However, accumulation of this tracer in the brain is limited. N-(2,5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide (DAA1106) was found to be a selective agonist for studying PBRs in the central nervous system (9, 10). DAA1106 was reported to have a higher affinity for PBRs in mitochondrial fractions of rat and monkey brains than did PK11195 (9, 10). Therefore, both tracers are able to cross the normal cell membrane to reach the mitochondrial receptor sites. N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^18^F]fluoroethyl-5-methoxybenzyl)acetamide ([^18^F]FEDAA1106) and [^11^C]DAA1106 have been developed as potential PET ligands with highly selective and specific binding to PBR (11, 12). N-Benzyl-N-ethyl-2-[7,8-dihydro-7-(2-[^18^F]fluoroethyl)-8-oxo-2-phenyl-9H-purin-9-yl]acetamide ([^18^F]FEAC), which has an acetamide structure, has been evaluated for imaging PBR in the brain (13).

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PBR%5BAll+Fields%5D+AND+micad%5Bbook%5D)
- Gene information in NCBI (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=706%5Buid%5D))
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=109610)
- Clinical trials (PBR (http://www.clinicaltrials.gov/ct2/results?term=pk11195+OR+PBR))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%20and%20synthesis)]

Yanamoto et al. (13) reported the synthesis of [^18^F]FEAC by alkylation of the precursor with [^18^F]FCH_2_CH_2_Br. [^18^F]FEAC was purified with high-performance liquid chromatography with 35% radiochemical yield (decay-corrected) based on [^18^F]F^-^. The total synthesis time was ~45 min. The radiochemical purity was >98% with the specific activity of 30–95 GBq/μmol (0.81–2.43 Ci/μmol) at the end of synthesis.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%20and%20in%20vitro)]

In vitro [^11^C]PK11195 PBR-binding studies using rat brain homogenates showed inhibition constant (K_i_) values of 0.49 ± 0.05 nM and 0.31 ± 0.03 nM for FEAC and PK11195, respectively (13). Log D was determined to be 3.6 and 3.7 for FEAC and PK11195, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%20and%20rodentia)]

Yui et al. (14) showed that [^18^F]FEAC had high accumulation as expressed in % injected dose/gram (ID/g) in the lung (35.3), heart (9.6), kidney (17.1), liver (9.3) and small intestine (5.4) in normal mice at 5 min after injection. The brain exhibited 1% ID/g at 1 min and ~0.45% for next 89 min. The radioactivity in the bone was 1.1% ID/g at 1 min and 1.4% ID/g at 90 min. PET imaging scans were performed in rats with infarcted brain. Maximum uptake (1-3 min after injection) on the ipsilateral and contralateral sides was about 0.87 and 0.49 standardized uptake value (SUV), respectively. The SUV ratio of radioactivity between ipsilateral and contralateral sides reached 3.03 for [^18^F]FEAC at 20 min after injection. The ratio was reduced to ~1 with PK11195 pretreatment (~1 min). The binding potential was estimated to be 1.70 ± 0.19 (n = 4).

Yanamoto et al. (13) performed PET imaging in rats (n = 4) with acute neuroinflammation in the striatum. PET imaging showed an increased accumulation of [^18^F]FEAC in the lesion as compared with the contralateral side as early as 1 min after injection with rapid clearance. The maximum ratio of 2.5 was achieved within 10–20 min after injection. No blocking experiment was performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%20and%20%28dog%20or%20sheep%20or%20pig%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%20and%20%28primate%20not%20human%29)]

PET imaging was performed in a male rhesus monkey (14). The maximum uptake (0.016% dose/mL) of [18F]FEAC in the occipital cortex was at ~5 min after injection. At 90 min after injection, the radioactivity decreased to 70% of the maximum.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEAC%20and%20human)]

No publications are currently available.

## References

1 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
2 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
6 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
7 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
8 Gerhard A., Neumaier B., Elitok E., Glatting G., Ries V., Tomczak R., Ludolph A.C., Reske S.N. (2000). In vivo imaging of activated microglia using [11C]PK11195 and positron emission tomography in patients after ischemic stroke. Neuroreport.
9 Okuyama S., Chaki S., Yoshikawa R., Ogawa S., Suzuki Y., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Neuropharmacological profile of peripheral benzodiazepine receptor agonists, DAA1097 and DAA1106. Life Sci.
10 Chaki S., Funakoshi T., Yoshikawa R., Okuyama S., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Binding characteristics of [3H]DAA1106, a novel and selective ligand for peripheral benzodiazepine receptors. Eur J Pharmacol.
11 Fujimura Y., Ikoma Y., Yasuno F., Suhara T., Ota M., Matsumoto R., Nozaki S., Takano A., Kosaka J., Zhang M.R., Nakao R., Suzuki K., Kato N., Ito H. (2006). Quantitative analyses of 18F-FEDAA1106 binding to peripheral benzodiazepine receptors in living human brain. J Nucl Med.
12 Maeda J., Suhara T., Zhang M.R., Okauchi T., Yasuno F., Ikoma Y., Inaji M., Nagai Y., Takano A., Obayashi S., Suzuki K. (2004). Novel peripheral benzodiazepine receptor ligand [11C]DAA1106 for PET: an imaging tool for glial cells in the brain. Synapse.
13 Yanamoto K., Kumata K., Yamasaki T., Odawara C., Kawamura K., Yui J., Hatori A., Suzuki K., Zhang M.R. (2009). [18F]FEAC and [18F]FEDAC: Two novel positron emission tomography ligands for peripheral-type benzodiazepine receptor in the brain. Bioorg Med Chem Lett.
14 Yui, J., J. Maeda, K. Kumata, K. Kawamura, K. Yanamoto, A. Hatori, T. Yamasaki, N. Nengaki, M. Higuchi, and M.R. Zhang, 18F-FEAC and 18F-FEDAC: PET of the Monkey Brain and Imaging of Translocator Protein (18 kDa) in the Infarcted Rat Brain. J Nucl Med, 2010